# 2-[^18^F]Fluoropropionyl-osteosarcoma–specific peptide-1 (ASGALSPSRLDT)

Chemical name: | 2-[^18^F]Fluoropropionyl-osteosarcoma–specific peptide-1 (ASGALSPSRLDT)
Abbreviated name: | [^18^F]FP-OSP-1
Synonym:
Agent Category: | Peptide
Target: | Heparan sulfate proteoglycans (HSPG)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OSP-1)]

Osteosarcoma typically affects adolescents and represents the most common primary bone tumor in childhood (1). Approximately 25% of osteosarcomas metastasize to the lung (2). Heparan sulfate proteoglycans (HSPGs) are glycoproteins that are glycosylated with two or three heparan sulfate polysaccharide chains. HSPGs are associated with the cell surface of cells (3). HSPGs play an important role in cell–cell and cell–extracellular matrix adhesion. Heparan sulfate binds to a variety of protein ligands (e.g., growth factors and interleukins) and regulates a wide variety of biological activities, including developmental processes, angiogenesis, blood coagulation, and tumor metastasis. HSPGs are overexpressed on a variety of tumor cells including osteosarcoma cells (4, 5). Sun et al. (6) identified a new 12-mer peptide (OSP-1, ASGALSPSRLDT) with the use of phage display screening against human osteosarcoma 143B cells with a high homology to the 17-28 amino acid residues of heparinase II/III. Heparinases bind and cleave cell-surface HSPGs. OSP-1 was radiolabeled with 4-nitrophenyl-2-[^18^F]fluoropropionic acid at the N-terminus to yield 2-[^18^F]fluoropropionyl-OSP-1 ([^18^F]FP-OSP-1), which was then evaluated for positron emission tomography (PET) imaging of tumor xenografts in mice.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=proteoglycans+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (HSPG (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6383)).
- Articles in OMIM (HSPG (http://www.ncbi.nlm.nih.gov/omim/142460))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OSP-1+synthesis)]

OSP-1 and its scrambled peptide OSP-S (DLPSRTSALASG) were prepared with solid-phase peptide synthesis (6). Peptide purity and molecular mass were confirmed with MALDI-TOF mass spectroscopy and electrospray ionization mass spectrometry. To label with ^18^F, OSP-1 was incubated with 4-nitrophenyl-2-[^18^F]fluoropropionic acid in dimethyl sulfoxide for 1 h at room temperature. [^18^F]FP-OSP-1 was purified with high-performance liquid chromatography with a radiochemical yield of 20% at the end of purification. The specific activity was ~37 GBq/µmol (1 Ci/µmol). Radiochemical purity of the injected product was not reported. [^18^F]FP-OSP-S was prepared similarly and had a similar radiochemical yield, radiochemical purity, and specific activity.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OSP-1+in+vitro+studies)]

Studies of the cellular uptake and efflux of [^18^F]FP-OSP-1 into 143B human osteosarcoma cell line (high HSPG expression), UM-SCC1 human neck and head squamous carcinoma cell line (low HSPG expression), and 293T human embryonic kidney cell line (low HSPG expression) cells were performed in culture (6). The accumulation was time-dependent with 0.4%, 0.2%, and 0.1% of the incubation dose in 143B, UM-SCC1, and 293T cells, respectively, after 60 min of incubation at 37°C. [^18^F]FP-OSP-S exhibited little uptake in 143B cells. 143B cells retained ~50% of radioactivity after 60 min, whereas the radioactivity in UM-SCC1 and 293T cells was undetectable after 60 min. Immuofluorescence staining with anti-heparin/heparin sulfate antibody showed strong binding to 143B cells but not to UM-SCC1 or 293T cells. Preincubation of 143B cells with OSP-1 abrogated the antibody binding.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OSP-1+rodentia)]

Sun et al. (6) performed ex vivo biodistribution studies of [^18^F]FP-OSP-1 (0.93 MBq (25 μCi)) at 2 h after intravenous injection in nude mice (n = 4/group) bearing 143B and UM-SCC1 xenografts. Tracer accumulation was significantly higher (P < 0.05) in 143B tumors (2.4 ± 0.1% injected dose per gram (ID/g)) than in UM-SCC1 tumors (1.2 ± 0.3% ID/g). The organ with the highest radioactivity was the intestine (1.3% ID/g). Accumulation in most normal organs was <1% ID/g. The radioactivity values in the blood and bone were 1% ID/g and 0.5% ID/g, respectively. Experiments with injection of [^18^F]FP-OSP-S showed that [^18^F]FP-OSP-S exhibited a significantly lower (P < 0.05) tracer accumulation in 143B tumors than [^18^F]FP-OSP-1 (1.1% ID/g versus 2.5% ID/g). The tumor/muscle ratios were 3.49 ± 0.35 and 1.74 ± 0.05 for [^18^F]FP-OSP-1 and [^18^F]FP-OSP-S at 2 h, respectively (P < 0.05).

PET analysis was performed after intravenous injection of 3.7 MBq (100 μCi) [^18^F]FP-OSP-1 or [^18^F]FP-OSP-S in nude mice (n = 6/group) bearing 143B and UM-SCC1 xenografts (6). The 143B tumors were clearly visualized with high contrast compared with the UM-SCC1 tumors at 0.5–2 h after injection of [^18^F]FP-OSP-1. Tumor accumulation was determined to be 1.43 ± 0.14% ID/g for 143B tumors and 0.75 ± 0.12% ID/g for UM-SCC1 tumors at 2 h after injection (P < 0.01). [^18^F]FP-OSP-1 accumulation was three- to five-fold higher than [^18^F]FP-OSP-S in 143B tumors at 0.5–2 h. The 143B tumor/muscle ratios were 3.77 ± 0.21 and 1.54 ± 0.18 for [^18^F]FP-OSP-1 and [^18^F]FP-OSP-S at 2 h, respectively (P < 0.05). The tumor/muscle ratios of [^18^F]FP-OSP-S were similar in 143B and UM-SCC1 tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=OSP-1%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OSP-1+Non+Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OSP-1+Human+Studies)]

No references are currently available.

## NIH Support

Intramural Research Program

## References

1 Lamoureux F., Trichet V., Chipoy C., Blanchard F., Gouin F., Redini F. (2007). Recent advances in the management of osteosarcoma and forthcoming therapeutic strategies. Expert Rev Anticancer Ther.
2 Scotlandi K., Picci P., Kovar H. (2009). Targeted therapies in bone sarcomas. Curr Cancer Drug Targets.
3 Lamoureux F., Baud'huin M., Duplomb L., Heymann D., Redini F. (2007). Proteoglycans: key partners in bone cell biology. Bioessays.
4 McQuillan D.J., Midura R.J., Hascall V.C., Yanagishita M. (1992). Plasma-membrane-intercalated heparan sulphate proteoglycans in an osteogenic cell line (UMR 106-01 BSP). Biochem J.
5 Nikitovic D., Zafiropoulos A., Tzanakakis G.N., Karamanos N.K., Tsatsakis A.M. (2005). Effects of glycosaminoglycans on cell proliferation of normal osteoblasts and human osteosarcoma cells depend on their type and fine chemical compositions. Anticancer Res.
6 Sun X., Niu G., Yan Y., Yang M., Chen K., Ma Y., Chan N., Shen B., Chen X. (2010). Phage display-derived peptides for osteosarcoma imaging. Clin Cancer Res.